# ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-c(RGDyK)-bombesin[7-14]

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-c(RGDyK)-bombesin[7-14]
Abbreviated name: | ^68^Ga-NOTA-RGD-BBN
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR), integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on CNS and GI tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (7). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (8-13). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various ligands have been introduced for imaging of tumors and tumor angiogenesis (14).

Because breast and prostate cancers express GRPR and α_v_β_3_, Liu et al. (15) designed an RGD-BBN heterodimer in which BBN[7-14] and c(RGDyK) are connected with a glutamate linker (BBN on the Glu side chain γ-carboxylate group and RGD on the Glu side chain α-carboxylate group). A spacer, 11-amino-3,6,9-trioxaundecanoic acid (PEG_3_), was put onto the glutamate α-amino group of Glu-RGD-BBN to increase the hydrophilicity and to relieve the steric hindrance. N-Succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) was used to synthesize [^18^F]FB-PEG_3_-RGD-BBN for tumor targeting. Liu et al. (16) used 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) as a bifunctional chelator for labeling RGD-BBN to form ^68^Ga-NOTA-RGD-BBN for positron emission tomography (PET) imaging of α_v_β_3_ and GRPR in nude mice bearing human tumors (15, 17).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=BBN%20and%20RGD+AND+micad%5Bbook%5D)
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=integrin%5BAll+Fields%5D)
- Clinical trials (Integrin (http://www.clinicaltrials.gov/ct2/results?term=integrin))
- FDA Drug information (Integrin (http://google2.fda.gov/search?q=Integrin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+synthesis)]

RGD-BBN was prepared with solid-phase peptide synthesis with subsequent addition of a NOTA group to form NOTA-RGD-BBN (15). Addition of a NOTA group to RGD-BBN was performed by mixing 2 µmol RGD-BBN with 6 µmol p-SCN-Bz-NOTA in sodium bicarbonate buffer (pH 9) for 5 h at room temperature. NOTA-RGD-BBN was isolated with high-performance liquid chromatography (HPLC) with 52% yield. Measurement with matrix-assisted laser desorption ionization time of flight mass spectrometry indicated the molecular mass to be m/z 2,235.3 (calculated molecular weight, 2,234.6). For ^68^Ga labeling, a solution of 148 MBq (4 mCi) ^68^Ga and 5 nmol NOTA-RGD-BBN in acetate buffer (pH 5) was heated for 15 min at 40°C (16). ^68^Ga-NOTA-RGD-BBN was purified with HPLC with a yield of 90% and a radiochemical purity of >98%. The specific activity was 7.4–14.8 GBq/µmol (0.2–0.4 Ci/µmol) at the end of synthesis. The total preparation time was ~45 min. ^68^Ga-NOTA-BBN and ^68^Ga-NOTA-RGD as controls were also prepared.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+in+vitro)]

Liu et al. (16) performed in vitro inhibition studies of NOTA-RGD-BBN in cultured U87MG cells with ^125^I-c(RGDyK). The 50% inhibition concentration (IC_50_) value was 22.6 ± 6.7 nM. The IC_50_ values for RGD-BBN and c(RGDyK) were 17.9 ± 5.7 and 11.2 ± 4.2 nM, respectively. In vitro inhibition studies of NOTA-RGD-BBN were also performed in cultured PC-3 cells with ^125^I-BBN, with an IC_50_ value of 55.9 ± 4.2 nM. The IC_50_ values for RGD-BBN and BBN were 67.9 ± 5.0 and 79.0 ± 4.9 nM, respectively. PC-3 cells exhibited 6.7%, 1.1% and 0.1% uptake of the incubation dose for ^68^Ga-NOTA-BBN, ^68^Ga-NOTA-RGD-BBN, and ^68^Ga-NOTA-RGD respectively, within 60 min of incubation at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+%20rodentia)]

Liu et al. (16) performed PET imaging of PC-3 tumor-bearing mice (n = 4/group) after injection of 3.7 MBq (100 uCi) of ^68^Ga-NOTA-BBN, ^68^Ga-NOTA-RGD-BBN, or ^68^Ga-NOTA-RGD. The estimated accumulation of ^68^Ga-NOTA-RGD-BBN in the tumors was 6.55 ± 0.83% injected dose per gram (ID/g) at 30 min, and it decreased to 5.26 ± 0.32% ID/g at 1 h and 4.04 ± 0.28% ID/g at 2 h after injection. The tumor accumulation of ^68^Ga-NOTA-RGD-BBN was higher that of ^68^Ga-NOTA-BBN, and ^68^Ga-NOTA-RGD at these time points (P < 0.05). The liver uptake of the three tracers were <2% ID/g at these time points. The kidney uptake of ^68^Ga-NOTA-RGD-BBN, and ^68^Ga-NOTA-BBN (9-10% ID/g) at 30 min after injection was higher than ^68^Ga-NOTA-RGD (5% ID/g) (P < 0.05). The tumor/muscle ratios were 6, 4, and 3 for ^68^Ga-NOTA-BBN, ^68^Ga-NOTA-RGD-BBN, and ^68^Ga-NOTA-RGD at 60 min after injection, respectively. In another study, BBN, c(RGDyK), or BBN+c(RGDyK) were co-injected with ^68^Ga-NOTA-RGD-BBN in mice bearing PC-3 tumors (n = 4/group). Tumor accumulation at 1 h after injection (5.26% ID/g) was only partially inhibited by either BBN (1.61% ID/g) or c(RGDyK) (2.08% ID/g) alone. However, BBN+c(RGDyK) reduced tumor accumulation to the background level (0.42% ID/g). PET scans were also performed after intravenous injection of 3.7 MBq (100 μCi) ^68^Ga-NOTA-BBN, ^68^Ga-NOTA-RGD-BBN, or ^68^Ga-NOTA-RGD in nude mice (n = 4/group) bearing MDA-MB-435 human breast tumors with moderate expression of including α_v_β_3_ and undetectable expression of GRPR at 60 min. The estimated accumulation in the MDA-MB-435 tumors was 0.38%, 3.23% and 1.63% ID/g at 60 min, respectively. Ex vivo biodistribution studies showed that the tissue with the highest accumulation was the pancreas, followed by the kidney, PC-3 tumor, intestine, stomach, liver, blood, and muscle at 0.5 and 1 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+human)]

No publication is currently available.

## NIH Support

R01 CA119053, R21 CA121842, P50 CA114747, U54 CA119367

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
7 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
8 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
9 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
10 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
11 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
12 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
13 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
14 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
15 Liu Z., Yan Y., Chin F.T., Wang F., Chen X. (2009). Dual integrin and gastrin-releasing peptide receptor targeted tumor imaging using 18F-labeled PEGylated RGD-bombesin heterodimer 18F-FB-PEG3-Glu-RGD-BBN. J Med Chem.
16 Liu Z., Niu G., Wang F., Chen X. (2009). (68)Ga-labeled NOTA-RGD-BBN peptide for dual integrin and GRPR-targeted tumor imaging. Eur J Nucl Med Mol Imaging.
17 Liu Z., Li Z.B., Cao Q., Liu S., Wang F., Chen X. (2009). Small-animal PET of tumors with (64)Cu-labeled RGD-bombesin heterodimer. J Nucl Med.